# Fluoro-pegylated (1E,4E)-1-(4-(dimethylamino)phenyl)-5-(4-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)phenyl)penta-1,4-dien-3-one and (1E,4E)-1-(4-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)phenyl)-5-(4-(methylamino)phenyl)penta-1,4-dien-3-one

Chemical name: | Fluoro-pegylated (1E, 4E)-1-(4-(dimethylamino)phenyl)-5-(4-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)phenyl)penta-1,4-dien-3-one and (1E, 4E)-1-(4-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)phenyl)-5-(4-(methylamino)phenyl)penta-1,4-dien-3-one | [image]
Abbreviated name: | [^18^F]83, [^18^F]85 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | β-amyloid (Aβ) | [image]
Target Category: | Accepters | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of [^18^F]83 and [^18^F]85 by Cui et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=molecular%20imaging%20and%20Alzheimer%u2019s%20disease%20and%20%u03B2-amyloid%20)]

Fluoro-pegylated (1E, 4E)-1-(4-(dimethylamino)phenyl)-5-(4-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)phenyl)penta-1,4-dien-3-one (compound 83) and (1E, 4E)-1-(4-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)phenyl)-5-(4-(methylamino)phenyl)penta-1,4-dien-3-one (compound 85), abbreviated as [^18^F]83 and [^18^F]85, respectively, are two dibenzylideneacetone derivatives synthesized by Cui et al. for positron emission tomography (PET) of Alzheimer’s disease (AD) by targeting β-amyloid (Aβ) plaques (1).

AD is characterized in pathology by the presence of extracellular Aβ plaques, intraneuronal neurofibrillary tangles, and neuronal loss in the cerebral cortex (2, 3). Of them, Aβ deposit is the earliest neuropathological marker and is relatively specific to AD and closely related disorders. Aβ plaques are composed of abnormal paired helical filaments 5–10 nm in size. These filaments are largely made of insoluble Aβ peptides that are 40 or 42 amino acids in length (4). Aβ peptides have been shown to be toxic to neurons, and the level of Aβ peptides is closely correlated with the cognitive decline in AD. These features of Aβ prompted investigators to develop Aβ-targeted agents for AD imaging.

Curcumin is the principal component of the Indian spice turmeric, and in structure it is composed of two aromatic rings connected by two α,β-unsaturated carbonyl groups (1). In 2001, investigators at the University of California, Los Angeles, reported that curcumin is effective against neurodegeneration, oxidative damage, and diffuse plaque deposition after Aβ infusion in animals (5, 6). The anti-AD effect of curcumin has been further demonstrated to be partially due to its specific binding with Aβ, whereby it could break apart Aβ aggregates. In 2006, Ryu et al. tested eight curcumin derivatives as Aβ-specific imaging probes (7). In general, these derivatives are poor in brain–blood barrier (BBB) penetration and are unstable in vivo (1, 7). The curcumin derivatives are quickly converted to unidentified polar products, which cannot cross the BBB. The methylene moiety between the two aromatic rings is responsible for the poor stability, whereas the two aromatic rings are responsible for the binding with Aβ plaques. To improve the stability and BBB-penetrating ability of curcumin, various modifications on the curcumin structure have recently been made, including deleting the active methylene moiety in the middle of its structure (1).

Cui et al. synthesized a series of dibenzylideneacetones by deleting the methylene moiety and one carbonyl moiety and further linking various substituents on one (forming an asymmetrical structure) or on both aromatic rings (forming a symmetrical structure) (1). Analysis of the structure–affinity relationship among these derivatives has shown that dibenzylideneacetone without any substituents have a weak affinity with Aβ (inhibition constant (K_i_) = 242.5 ± 42.8 nM). Introduction of Cl or methoxy groups at the para position on both phenyl rings to form symmetrical ligands can significantly increase the binding affinity (~90 folds), and the size of substituents has no effect on the affinity for Aβ aggregates. Methylation of a primary amino group to form a secondary or tertiary amino group can also significantly increase the affinity (e.g., the agents [^125^I]70 and [^125^I]71 in MICAD), but methylation of the amino group at the ortho position reduces the binding affinity dramatically. Increasing the substituent size at the aromatic amino group also leads to decreased binding affinity. However, when a phenyl ring in the dibenzylideneacetone structure is changed to a heterocyclic ring, such as a thiophene, furan, pyridine, or pyrrole ring, the generated compounds maintain the high binding affinity. These results demonstrate that the para position is highly tolerant of steric bulk substitutions, which opens up the possibility of developing new, easily labeled radioligands for imaging Aβ plaques in vivo (1).

This chapter summarizes the data obtained with ^18^F]83 and [^18^F]85, two fluoro-pegylated dibenzylideneacetones (1). Another chapter summarizes the data obtained with [^125^I]70 and [^125^I]71, two asymmetrical dibenzylideneacetones with methylation of a primary amino group at the para position.

### Related Resource Links:

- Amyloid-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amyloid+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)
- Amyloid-targeted imaging clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=amyloid)
- Structures and other information of amyloid peptides in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=amyloid)
- Alzheimer’s disease articles in Online Mendelian Inheritance in Man (http://www.ncbi.nlm.nih.gov/omim/?term=Alzheimer%27s%20disease)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

Synthesis of the compound precursors was described in detail by Cui et al. (1). To generate [^18^F]83, the tosylate precursor 80 was mixed with [^18^F]fluoride/potassium carbonate and Kryptofix2.2.2 in dimethyl sulfoxide for 5 min under heating at 120°C. The mixture was purified with high-performance liquid chromatography. To generate [^18^F]85, the N-Boc-protected mesylate precursor was first treated with aqueous HCl to remove the N-Boc-protecting group. The radiochemical purity of both [^18^F]83 and [^18^F]85 was >98%. The radiochemical yields (decay-corrected) of [^18^F]83 and [^18^F]85 were 49% and 13%, respectively. The partition coefficients of [^18^F]83 and [^18^F]85 were 2.97 and 3.08, respectively, indicating that both agents were lipophilic. The specific activity for both [^18^F]83 and [^18^F]85 was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

The binding affinity of unlabeled compounds 83 and 85 for Aβ_1_−_42_ was examined with [^125^I]IMPY (6-iodo-2-(4'-dimethylamino)phenyl-imidazo[1,2]pyridine) as the competing radioligand (1, 8). The K_i_ values of compounds 83 and 85 were 6.9 ± 1.4 nM and 8.6 ± 1.3 nM, respectively, which was superior to the binding affinity of IMPY (K_i_ = 10.5 nM) (8).

The binding of [^18^F]83 and [^18^F]85 to Aβ plaques in brain tissue sections of transgenic mice (APP/PS1) was evaluated in vitro with autoradiography (1). Both ligands showed effective labeling of the plaques with minimal background, consistent with the findings from thioflavin S staining. The brain sections from normal mice were void of any notable Aβ labeling.

Autoradiographic studies of [^18^F]83 and [^18^F]85 were also performed in human AD brain sections to test their binding with human Aβ plaques (1). Specific labeling of the plaques was observed, and immunohistochemical staining confirmed the presence of plaques in the sections.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

Biodistribution of [^18^F]83 and [^18^F]85 was analyzed in normal mice (n = 4/time point for each agent) (1). Both [^18^F]83 and [^18^F]85 exhibited good initial penetration of the BBB with initial brain uptakes of 4.13% and 5.15% ID/g at 2 min after injection, respectively, showing improved initial uptake than the previously reported radiofluorinated curcumin (0.52% ID/g at 2 min) (7). The radioactivity was then washed out rapidly (0.90% and 1.27% ID/g at 60 min for [^18^F]83 and [^18^F]85, respectively). The brain_2min_/brain_60min_ ratios were 4.59 and 4.06 for [^125^I]70 and [^125^I]71, respectively. The defluorination, as reflected by bone uptake, was low (2.33% and 2.54% ID/g in the bone at 1 h for [^18^F]83 and [^18^F]85, respectively). Both agents were cleared predominantly by the hepatobiliary system (14.07% and 19.24% ID/g in the liver at 30 min for [^18^F]83 and [^18^F]85, respectively). The hepatobiliary excretion to the intestines was also rather fast, and radioactivity was observed to accumulate within the intestines at later time points (21.57% and 26.26% ID/g in the intestines at 60 min for [^18^F]83 and [^18^F]85, respectively). A moderate uptake of the two agents was also observed in the kidneys (7.13% and 11.51% ID/g at 30 min for [^18^F]83 and [^18^F]85, respectively), indicating that they were also excreted via the renal system.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

No references are currently available.

## References

1 Cui M., et al. (2011). Synthesis and structure-affinity relationships of novel dibenzylideneacetone derivatives as probes for beta-amyloid plaques. J Med Chem.
2 Ono M. (2009). Development of positron-emission tomography/single-photon emission computed tomography imaging probes for in vivo detection of beta-amyloid plaques in Alzheimer's brains. Chem Pharm Bull (Tokyo).
3 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
4 Vallabhajosula S. (2011). Positron emission tomography radiopharmaceuticals for imaging brain Beta-amyloid. Semin Nucl Med.
5 Frautschy S.A., et al. (2001). Phenolic anti-inflammatory antioxidant reversal of Abeta-induced cognitive deficits and neuropathology. Neurobiol Aging.
6 Lim G.P., et al. (2001). The curry spice curcumin reduces oxidative damage and amyloid pathology in an Alzheimer transgenic mouse. J Neurosci.
7 Ryu E.K., et al. (2006). Curcumin and dehydrozingerone derivatives: synthesis, radiolabeling, and evaluation for beta-amyloid plaque imaging. J Med Chem.
8 Newberg A.B., et al. (2006). Safety, biodistribution, and dosimetry of 123I-IMPY: a novel amyloid plaque-imaging agent for the diagnosis of Alzheimer's disease. J Nucl Med.